# ^111^In-Diethylenetriamine pentaacetic acid-Anti-ligand–induced binding sites (LIBS) single-chain (scFv) antibody

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-Anti-ligand–induced binding sites (LIBS) single-chain (scFv) antibody
Abbreviated name: | ^111^In-DTPA-LIBS-scFv
Synonym:
Agent category: | Antibody, single-chain
Target: | Platelet glycoprotein GPIIb/IIIa receptor (CD61/CD41)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS)]

Thrombosis plays a major role in many cardiovascular diseases, such as myocardial infarction, pulmonary embolism (PE), deep venous thrombosis (DVT), atherothrombosis, or cerebral venous thrombosis (1, 2). DVT is a significant cause of PE, which is a potentially life-threatening clinical problem. Thrombosis occurs when platelets deposit in regions of low flow in the deep venous system, followed by an activation process of thrombin, which then converts fibrinogen into fibrin. Platelets become activated and bind to fibrinogen, resulting in platelet aggregation via the platelet integrin GPIIb/IIIa (α_IIb_β_3_, CD61/CD41). The thrombus may become organized or may detach from the vessel wall. A single-chain antibody (scFv) anti-LIBS-scFv was developed to recognize ligand-induced binding sites (LIBS) epitope of GPIIb/IIIa on the platelets that become exposed only upon activation (3). Anti-LIBS-scFv does not bind to circulating platelets. Heidt et al. (4) evaluated ^111^In-diethylenetriamine pentaacetic acid-anti-LIBS-scFv (^111^In-DTPA-LIBS-scFv) as an ^111^In-based single-photon emission computed tomography (SPECT) agent for imaging platelet-containing thrombus.

### Related Resource Links:

- Chapters in MICAD (GPIIb (http://www.ncbi.nlm.nih.gov/books?term=GPIIb%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), thrombus (http://www.ncbi.nlm.nih.gov/books?term=thrombus%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/gene/3690), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/gene/3674))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GPIIIa/CD61 (http://omim.org/entry/173470), GPIIb/CD41 (http://omim.org/entry/607759))
- Clinical trials (integrin (http://www.clinicaltrials.gov/ct2/results?term=integrin))
- Drug information in FDA (integrin (http://google2.fda.gov/search?q=integrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS+and+synthesis)]

DTPA-LIBS-scFv was prepared by conjugation of excess p-isothiocyanatobenzyl-DTPA to LIBS-scFv (7.7 nmol) for 60 min at 25°C (4). DTPA-LIBS-scFv was purified with filtration. DTPA-LIBS-scFv (1.5 nmol) was incubated with 20 MBq (0.54 mCi) ^111^InCl_3_ in 0.25 M NH_4_Ac buffer (pH 5.4) for 30 min at 25°C. ^111^In-DTPA-LIBS-scFv was purified with filtration. ^111^In-Labeling efficiency was 68.8 ± 8.7% with >90% radiochemical purity. The specific activity of ^111^In-DTPA-LIBS-scFv and the number of DTPA moieties per scFv were not reported. ^111^In-DTPA-control-scFv was prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS+and+in+vitro)]

Flow cytometry analysis showed that DTPA-control-scFv had no binding to adenosine diphosphate-activated or nonactivated platelets (4). On the other hand, DTPA-LIBS-scFv exhibited an increase in binding in activated platelets compared with nonactivated platelets. Autoradiographic imaging studies of activated platelets were performed with ^111^In-DTPA-LIBS-scFv and ^111^In-DTPA-control-scFv. ^111^In-DTPA-LIBS-scFv exhibited a significantly higher radioactivity (4,520 ± 293 digital light units/mm^2^ (DLU/mm^2^)) than ^111^In-DTPA-control-scFv (1,866 ± 246 DLU/mm^2^) (P < 0.05, n = 6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS+and+rodentia)]

Heidt et al. (4) performed ex vivo autoradiographic imaging of thrombosis in mice (n = 5 mice/group) exposed to 6.5% ferric chloride solution to injure the carotid artery at 30 min after injection of ~1 MBq (0.027 mCi, 0.4 nmol) ^111^In-DTPA-LIBS-scFv or ^111^In-DTPA-control-scFv. ^111^In-DTPA-LIBS-scFv exhibited a significant increase in radioactivity at the side of the intravascular thrombosis (49,630 ± 10,650 DLU/mm^2^) compared to the contralateral non-injured side (17,390 ± 7,470 DLU/mm^2^) (P < 0.05). On the other hand, ^111^In-DTPA-control-scFv revealed low radioactivity at these two sides (1,736 ± 522 DLU/mm^2^versus 1,373 ± 385 DLU/mm^2^, respectively). No blocking studies were performed.

Heidt et al. (4) performed in vivo SPECT/CT imaging of the injured carotid artery in mice (n = 4 mice/group) at 30 min after injection of ~15 MBq (0.4 mCi) ^111^In-DTPA-LIBS-scFv or ^111^In-DTPA-control-scFv. Region-of-interest analysis of the thrombosis showed that ^111^In-DTPA-LIBS-scFv resulted in a target/background ratio of 1.99 ± 0.36, which was significantly higher than that of ^111^In-DTPA-control-scFv (1.10 ± 0.24) (P < 0.01). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DTPA%20LIBS+and+human)]

No publication is currently available.

## References

1 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
2 Taillefer R. (2001). Radiolabeled peptides in the detection of deep venous thrombosis. Semin Nucl Med.
3 Schwarz M., Meade G., Stoll P., Ylanne J., Bassler N., Chen Y.C., Hagemeyer C.E., Ahrens I., Moran N., Kenny D., Fitzgerald D., Bode C., Peter K. (2006). Conformation-specific blockade of the integrin GPIIb/IIIa: a novel antiplatelet strategy that selectively targets activated platelets. Circ Res.
4 Heidt T., Deininger F., Peter K., Goldschmidt J., Pethe A., Hagemeyer C.E., Neudorfer I., Zirlik A., Weber W.A., Bode C., Meyer P.T., Behe M., von Zur Muhlen C. (2011). Activated platelets in carotid artery thrombosis in mice can be selectively targeted with a radiolabeled single-chain antibody. PLoS One.